# Protoporphyrin IX and IR-820 fluorophore–encapsulated organically modified silica nanoparticles

Chemical name: | Protoporphyrin IX and IR-820 fluorophore–encapsulated organically modified silica nanoparticles
Abbreviated name: | PpIX/IR-820–doped ORMOSIL NPs
Synonym:
Agent Category: | Nanoparticles
Target: | Non-targeted
Target Category: | Non-targeted
Method of detection: | Optical imaging
Source of signal / contrast: | IR-820
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=organically%20modified%20silica%20nanoparticles)]

Protoporphyrin IX (PpIX) and IR-820 fluorophore–encapsulated organically modified silica nanoparticles (ORMOSIL NPs), abbreviated as PpIX/IR-820–doped ORMOSIL NPs, were synthesized by Qian et al. for two-photon photodynamic therapy (PDT) and optical imaging (1).

PDT has been investigated for several decades as an alternative to chemotherapy and radiotherapy for tumor treatment (2, 3). PDT involves the use of light, a photosensitizer (PS), and tissue oxygen. Under light excitation, PS transfers its energy to neighboring oxygen molecules, resulting in the generation of singlet oxygen (^1^O_2_) and other cytotoxic reactive oxygen species, which leads to apoptosis and necrosis of cancer cells. To date, most PSs developed for PDT are hydrophobic, aggregate easily in blood, and exhibit poor tumor selectivity (1, 2). One technique to overcome these issues is to link PSs to or encapsulate them in nanocarriers (4, 5).

Nanocarriers have been synthesized with diverse nanomaterials such as polymers, metals, semi-conductors, and silica. ORMOSIL NPs have shown great potential as an ideal nano-platform for theranostic applications because of their unique properties (6-8). First, ORMOSIL NPs are chemically inert, and the silica matrix porosity is resistant to swelling or changes in varying pH conditions. Second, ORMOSIL NPs can be loaded with both hydrophilic and hydrophobic payloads and protected from degradation by the bio-environment. PSs can be encapsulated in the monomeric form without loss of activity. Third, ORMOSIL NPs are mesoporous, which allows controlled release of the encapsulated biomolecules. Fourth, ORMOSIL NPs are able to accumulate selectively in tumors through the enhanced permeability and retention effects of tumor tissues. Finally, the size, shape, porosity, and monodispersibility of the ORMOSIL NPs can be controlled during preparation, and their surfaces can be functionalized with various chemical groups and/or targeting biomolecules.

The most recent studies on PDT with ORMOSIL NPs have focused on the targeted delivery for two-photon PDT in deep tissues and on the multimodal applications within one NP platform, such as the combination of magnetic resonance imaging, optical imaging, and PDT (2, 3). For imaging and therapeutic purposes, Qian et al. synthesized PpIX-doped and near-infrared (NIR) dye IR-820–doped ORMOSIL NPs (1). PpIX is a photosensitizer currently used in the clinic. The investigators tested the feasibility of using the NPs for optical imaging and PDT of tumor cells under two-photon excitation (1).

### Related Resource Links:

Photodynamic therapy-related imaging probes in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=photodynamic+therapy+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Photodynamic therapy clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=photodynamic+therapy)

Silica nanoparticle-based imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=silica+nanoparticles++AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22484045)]

PpIX/IR-820–doped ORMOSIL NPs were synthesized by Qian et al. in the nonpolar core of Aerosol-OT/DMSO/water micelles (1). The NPs were further modified with polyethylene glycol. At the end of synthesis, both PpIX-doped and IR-820–doped ORMOSIL NPs had a narrow size distribution with an average diameter of ~25 nm and ~42 nm, respectively. Both types of NPs showed a spherical morphology with a mesoporous matrix on their surface under transmission electron microscopy. The strongest linear absorption band of PpIX-doped ORMOSIL NPs was ~404 nm, and its decaying tail extended into the 600–650 nm range. Spectral studies on IR-820–doped ORMOSIL NPs showed absorption and emission values of 700–900 nm and 836–850 nm, respectively. The amount of each payload per NP was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22484045)]

Two-photon imaging of PpIX-doped ORMOSIL NPs in HeLa cells was performed with a two-photon confocal microscope under 800-nm femtosecond laser excitation after incubation of HeLa cells with PpIX-doped ORMOSIL NPs for 2 h at 37°C (1). Confocal microscopy showed bright red fluorescent signal distributed within the cells, which was from the intracellular PpIX. There was no obvious aggregation of the NPs in cell culture conditions.

The two-photon PDT efficacy of PpIX-doped ORMOSIL NPs was analyzed with HeLa cells and with 2 min irradiation under 800-nm laser from the confocal microscope (1). The HeLa cells treated with PpIX-doped ORMOSIL NPs showed no morphological changes immediately after 2 min irradiation. At 8 min after irradiation, the HeLa cells became round, and bubble-like changes were observed on the cell surface. These changes became more obvious over time, and at 15 min after irradiation, some cells started to show signs of necrosis. For the control HeLa cells without treatment, no obvious changes in their morphology were observed after irradiation. These results indicate that the two-photon excited PpIX led to the death of HeLa cells.

The imaging capacity of IR-820–doped ORMOSIL NPs in deep tissues was evaluated with a liquid phantom (1). The phantom was composed of intralipid and black ink, which had optical properties (especially in the NIR spectra) similar to typical human tissue. The IR-820–doped ORMOSIL NPs were buried in the phantom solution at different depths (0.5 cm, 1 cm, and 1.5 cm). NIR images showed that the NIR signal intensity decreased with increasing depth of the samples. The signal at a depth of 1.5 cm was still strong (280 units), and the image showed a high contrast without broadening compared to that at a depth of 0.5 cm.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22484045)]

The in vivo imaging efficiency of IR-820–doped ORMOSIL NPs was evaluated by Qian et al. with three animal models (n =1 mouse/model) (1). The investigators first applied the NPs for mouse brain imaging. The NPs (0.5 μl/location) were injected into the brain of a black mouse at depths of ~1 mm, 2 mm, 3 mm, and 4 mm, respectively. The four distinct NIR fluorescent points inside the brain could be clearly distinguished with optical imaging. The brightness of the fluorescence signal decreased at deeper locations.

Qian et al. then applied the NPs for sentinel lymph node (SLN) mapping (1). The NPs (0.1 ml) were injected intradermally into the forepaw pad of a nude mouse. At 4 min after injection, the fluorescence signal was observed at an axillary node, and the signal became stronger over time. At 20 min after injection, the signal intensity in the lymph node reached the maximum. The lymph node, which was dissected, emitted NIR fluorescence with a peak wavelength of 850 nm, consistent with that of IR-820–doped ORMOSIL NPs. These results suggested that IR-820–doped ORMOSIL NPs could be used as an NIR optical probe for in vivo SLN mapping.

Qian et al. further applied the NPs for tumor imaging (1). The NPs were injected via the tail vein into a nude mouse bearing a subcutaneous tumor xenograft (HeLa cells). At 5 h after injection, distinct NIR signals were observed in the liver, tumor, and tail. At 24 h, NIR fluorescence was still clear and distinct in the tumor and liver. After 10 days, the fluorescence could be observed clearly in the tumor, but not in the liver. After 30 days, the NPs in the tumor were cleared, and no more NIR signal could be observed. These results indicated that the NPs could home on mouse tumor xenographs, and that, due to the protection of the ORMOSIL NPs, the fluorescent dye remained stable for a relatively long time. No effects of the NPs were observed on the weight, shape, eating, drinking, or exploratory behavior of the mouse. For the control mouse without NP treatment, only autofluorescence was detected.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22484045)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22484045)]

No references are currently available.

## References

1 Qian J., Wang D., Cai F., Zhan Q., Wang Y., He S. (2012). Photosensitizer encapsulated organically modified silica nanoparticles for direct two-photon photodynamic therapy and in vivo functional imaging. Biomaterials.
2 Allison R.R., Bagnato V.S., Sibata C.H. (2010). Future of oncologic photodynamic therapy. Future Oncol.
3 Couleaud P., Morosini V., Frochot C., Richeter S., Raehm L., Durand J.O. (2010). Silica-based nanoparticles for photodynamic therapy applications. Nanoscale.
4 Baba K., Pudavar H.E., Roy I., Ohulchanskyy T.Y., Chen Y., Pandey R.K., Prasad P.N. (2007). New method for delivering a hydrophobic drug for photodynamic therapy using pure nanocrystal form of the drug. Mol Pharm.
5 Verhille M., Couleaud P., Vanderesse R., Brault D., Barberi-Heyob M., Frochot C. (2010). Modulation of photosensitization processes for an improved targeted photodynamic therapy. Curr Med Chem.
6 Ohulchanskyy T.Y., Roy I., Goswami L.N., Chen Y., Bergey E.J., Pandey R.K., Oseroff A.R., Prasad P.N. (2007). Organically modified silica nanoparticles with covalently incorporated photosensitizer for photodynamic therapy of cancer. Nano Lett.
7 Hocine O., Gary-Bobo M., Brevet D., Maynadier M., Fontanel S., Raehm L., Richeter S., Loock B., Couleaud P., Frochot C., Charnay C., Derrien G., Smaihi M., Sahmoune A., Morere A., Maillard P., Garcia M., Durand J.O. (2010). Silicalites and Mesoporous Silica Nanoparticles for photodynamic therapy. Int J Pharm.
8 Cheng S.H. (2011). andLo, L.W. Inorganic nanoparticles for enhanced photodynamic cancer therapy. Curr Drug Discov Technol.